# HSV1-TK/GFP/Fluc

Chemical name: | HSV1-TK/GFP/Fluc
Abbreviated name: | TGL
Synonym: | TGL triple reporter
Agent category: | Protein
Target: | Other
Target category: | Other – gene expression
Method of detection: | Optical imaging, gamma imaging, SPECT
Source of signal/contrast: | Green fluorescence protein (GFP), firefly luciferase, and ^131^I-FIAU
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HSV1-tk + GFP + luciferase)]

Reporter genes, also known as marker genes, possess a measurable phenotype distinguishable from the background of endogenous proteins (1). Several reporter genes express proteins that can generate signals for in vivo imaging, such as the herpes simplex virus type 1 thymidine kinase (HSV1-TK) gene, the green fluorescence protein (GFP) gene, and the firefly luciferase (Fluc) gene (2). The reporter gene is constructed with a “constitutive” promoter for continuous transcriptions or with an “inducible” promoter for controlled transcriptions (3). Both types of gene constructs have been used in the expression of exogenous genes and/or endogenous genes to monitor the levels of gene delivery and the efficiency in cell/tissue transduction in gene therapy.

HSV1-TK/GFP/Fluc (TGL, Mw = 130 kDa) is a triple reporter protein used for multimodal in vivo imaging of gene expression (4) with single photon emission computed tomography (SPECT) or fluorescence and bioluminescence imaging. TGL is produced from the expression of a triple-fusion reporter gene (TGL gene) in which transcription and translation are processed through a single open reading frame. TGL consists of three fused protein subunits: HSV1-TK, GFP, and Fluc, where polylysine is used as a linker to connect the protein subunits and to maintain the molecular stability in the fused protein. Each subunit corresponds to a specific imaging modality. HSV1-TK is a homodimer composed of two 376-residue subunits (5), and it functions as a key enzyme in the pyrimidine-salvage pathway to catalyze the phosphorylation of thymidine (dT) to thymidine monophosphate (dTMP) in the presence of ATP and Mg^2+^. This feature has been used to design antiviral nucleoside analogs (i.e., ganciclovir) for antiviral therapy (5) and radiolabeled substrates such as radiolabeled 2’-fluoro-2’-deoxy-1-β-D-arabino-furanosyl-5-iodo-uracil (FIAU) for SPECT imaging (6). HSV can easily infect a variety of cells in that the expressed HSV1-TK can induce significant cytotoxicity in the presence of nucleoside analogs such as ganciclovir (7). For this reason, HSV1-TK gene is also widely used as a suicide gene in cancer treatment. ^131^I-Labeled FIAU is an active radiolabeled substrate of HSV1-TK that is detectable with SPECT (i.e., ^131^I emits gamma-ray at 364 keV (81% abundance) with a half-life time of 8.02 days, which can be detected with a gamma camera or SPECT. GFP is a fluorescent protein of 238 amino acids that emits a bright green fluorescence (λ_max_ = 509 nm) when illuminated with a blue light (λ_max_ = 395 nm) (8). The presence of the GFP subunit allows in vitro/in vivo fluorescence imaging and cell sorting with the fluorescence-activated cell sorting (FACS) technique. Fluc is an oxygenase (Mw = 62 kDa) extracted from Photinus pyralis (9). In the presence of adenosine triphosphate (ATP) and O_2_, Fluc oxidizes the heterocyclic substrate D-luciferin to oxyluciferin and emits light in the wavelength range of 400–620 nm (10). The Fluc subunit allows for planar whole-body bioluminescence imaging of gene-transduced cells.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( HSV1-tk + GFP + luciferase)+AND+synthesis%0D%0A)]

Ponomarev et al. described the preparation of the HSV1-TK/GFP/Fluc expression vector in multiple steps (4). First, a construct SFG-HSV1-TK/GFP was obtained (11). Plasmid pLTKRNL was digested with restriction enzyme BamHI to generate a 2.2-kb fragment that encoded the open reading frame of HSV1-TK. This fragment was ligated into plasmid pcDNA.1/Zeo to result in the 7.8-kb plasmid pTKZeo3.2; this ligation was followed by sequential digestions with BamHI and Xmal to produce a 1.2-kb TK fragment. At the same time, plasmid pEGFP-N1 was digested sequentially with BgIII and Xmal to generate a 4.7-kb DNA fragment containing the open reading frame of GFP. The 1.2-kb fragment was then ligated with the 4.7-kb fragment to form the 5.9-kb expression plasmid pTKGFP, in which the TK-GFP cDNA was under control of the cytomegalovirus immediately early (IE) promoter. After the ligation, the plasmid was cloned into a retroviral vector, the Moloney murine leukemia virus-based SFG vector, to yield SFG-TK-GFP. Second, two modified constructs, SFG-NES-HSV1-TK/GFP and SFG-Δ45-HSV1-TK/GFP, were obtained (6). To generate SFG-NES-HSV1-TK/GFP, the Xenopus cDNA for encoding the 20 amino acids in the nuclear export signal (NES) sequence of the mitogen-activated protein (MAP) kinase kinase (MAPKK) was inserted into the N-terminus of HSV1-TK/GFP between His-9 and Ala-10 using MluL. To generate SFG-Δ45-HSV1-TK/GFP, the Δ45-HSV1 cDNA lacking the first 45 amino acids (135 nucleotides) of the original HSV1-TK was amplified with selective primers and subsequently cloned between the Ncol sites of SFG-HSV1-TK/GFP. Third, the commercially available cDNA of fused Aequorea victoria eGFP and Fluc (eGFP/Fluc) was obtained from the plasmid pEGF/Pluc and subcloned into the retroviral vector SFG-Ntp to yield the construct SFG-GL (4). Finally, SFG-NES-HSV1-TK/GFP or SFG-Δ45-HSV1-TK/GFP was treated with Ncol and the fragment containing NES-HSV1-TK or Δ45-HSV1-TK was subcloned into the NcoI site of the SFG-GL to produce SFG-NES-HSV1-TK/GFP/Fluc (SFG-NES-TGL) or SFG-Δ45-HSV1-TK/GFP/Fluc (SFG-Δ45-TGL) (4). [^131^I]-FIAU with >97% radiochemical purity was prepared by the iododestannylation reaction using the tin precursor and carrier-free ^131^I.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( HSV1-tk + GFP + luciferase)+AND+%22in+vitro%22)]

Ponomarev et al. assessed the integrity of the fused reporter proteins with Western blot analysis (4). The molecular weight of the NES-TGL and Δ45-TGL proteins as determined with Western blot analysis matched the predicted molecular weights. These proteins were further examined with anti-HSV1-TK, anti-GFP, and anti-Fluc antibodies to demonstrate the coexistence of the triple subunits in the full reporter proteins. Ponomarev et al. then imaged the cytoplasmic localizations of the NES-TGL and Δ45-TGL reporter proteins with fluorescence microscopy (4). Human glioma U87 cells were transduced with the retroviral vectors SFG-NES-TGL or SFG-Δ45-TGL in vitro, followed by a bulk culture for 48 h. The obtained U87-NES-TGL cells or U87-Δ45-TGL cells were sorted for positive GFP expression using FACS with 488-nm excitation beam and 510-nm emission filter. The subcellular localization of NES-TGL and Δ45-TGL was visualized with fluorescence microscopy with similar excitation emission parameters. The GFP/Fluc signal appeared to be lower in the nucleus than in cytoplasm, but it was still detectable. Reporter gene expression in these transduced U87 cells was quantified with FACS, a bioluminescence assay, and a radiotracer [^14^C]-FIAU assay. The level of GFP fluorescence was found to be ~1.3 × 10^3^ relative fluorescent units (RU) in the U87-NES-TGL cells and ~2.1 × 10^3^ RU in the U87-Δ45-TGL cells. The influx rate constant Ki of ^14^C-labeled FIAU was ~1.4 media ml/min per g in the U87-NES-TGL cells and ~1.7 media ml/min per g in the U87-Δ45-TGL cells. The bioluminescence was ~2.8 × 10^3^ relative bioluminescence unit (RLU) in the U87-NES-TGL cells and ~4.9 × 10^3^ RLU in the U87-Δ45-TGL. The wild-type U87 cells were used as a control. Their measured fluorescence, influx rate, and bioluminescence were negligible.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( HSV1-tk + GFP + luciferase) +AND++rodentia)]

Ponomarev et al. used three imaging modalities to examine the expression of the triple reporter proteins in vivo (4). Nu/nu mice (20–25 g) were implanted subcutaneously with U87-NES-TGL cells on the right shoulder, with U87-Δ45-TGL cells on the left shoulder, and with wild-type U87 cells on the left flank. The tumors grew to an average size of 5.4 ± 2.1 mm and were imaged with whole-body fluorescence, bioluminescence, and gamma camera imaging. For bioluminescence imaging, mice were injected intravenously with 100 μl of D-luciferin solution at a dose of 150 mg/kg, and the images were acquired for 0.5–10 s. For the gamma camera imaging, mice received an intraperitoneal injection of 0.9% NaI solution (1 ml) one day before imaging to block the thyroid uptake of radioactive iodide. Then the mice were injected intravenously with [^131^I]-FIAU at a dose of 7.4 MBq per animal. The gamma camera images were collected 24 h after [^131^I]-FIAU injection to allow sufficient clearance of body background radioactivity. The GFP fluorescence was collected with a charge-coupled device (CCD) camera. The average level of gene expression in the implanted U87-NES-TGL tumor was detected as 707 ± 36 in fluorescence, 486 ± 47 × 10^6^ photons/cm^2^ per sr in bioluminescence, and 0.47 ± 0.08% injected dose (ID)/g in [^131^I]-FIAU accumulation. The average level of gene expression in the implanted U87-Δ45-TGL tumor was detected as 740 ± 47 in fluorescence, 508 ± 36 × 10^6^ photons/cm^2^ per sr in bioluminescence, and 0.86 ± 0.06% ID/g in [^131^I]-FIAU accumulation. As a control, the average level of gene expression in the implanted wild-type U87 cells was found at background level in fluorescence or bioluminescence imaging and at 0.03 ± 0.01% ID/g in [^131^I]-FIAU accumulation (the background level). After completion of the triple modality imaging, the mice were euthanized and the tissues were harvested for in vitro fluorescence imaging. Bright green fluorescent areas were found in the tumor tissues, demonstrating the presence of TGL labeling.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( HSV1-tk + GFP + luciferase) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( HSV1-tk + GFP + luciferase) +AND+human)]

No publication is currently available.

## References

1 Massoud T.F., Singh A., Gambhir S.S. (2008). Noninvasive molecular neuroimaging using reporter genes: part I, principles revisited. AJNR Am J Neuroradiol.
2 Gross S., Piwnica-Worms D. (2005). Spying on cancer: molecular imaging in vivo with genetically encoded reporters. Cancer Cell.
3 Serganova I., Ponomarev V., Blasberg R. (2007). Human reporter genes: potential use in clinical studies. Nucl Med Biol.
4 Ponomarev V., Doubrovin M., Serganova I., Vider J., Shavrin A., Beresten T., Ivanova A., Ageyeva L., Tourkova V., Balatoni J., Bornmann W., Blasberg R., Gelovani Tjuvajev J. (2004). A novel triple-modality reporter gene for whole-body fluorescent, bioluminescent, and nuclear noninvasive imaging. Eur J Nucl Med Mol Imaging.
5 Wurth C., Thomas R.M., Folkers G., Scapozza L. (2001). Folding and self-assembly of herpes simplex virus type 1 thymidine kinase. J Mol Biol.
6 Ponomarev V., Doubrovin M., Serganova I., Beresten T., Vider J., Shavrin A., Ageyeva L., Balatoni J., Blasberg R., Tjuvajev J.G. (2003). Cytoplasmically retargeted HSV1-tk/GFP reporter gene mutants for optimization of noninvasive molecular-genetic imaging. Neoplasia.
7 Kussmann-Gerber S., Kuonen O., Folkers G., Pilger B.D., Scapozza L. (1998). Drug resistance of herpes simplex virus type 1--structural considerations at the molecular level of the thymidine kinase. Eur J Biochem.
8 Chalfie M., Tu Y., Euskirchen G., Ward W.W., Prasher D.C. (1994). Green fluorescent protein as a marker for gene expression. Science.
9 Conti E., Franks N.P., Brick P. (1996). Crystal structure of firefly luciferase throws light on a superfamily of adenylate-forming enzymes. Structure.
10 Paulmurugan R., Gambhir S.S. (2005). Firefly luciferase enzyme fragment complementation for imaging in cells and living animals. Anal Chem.
11 Jacobs A., Dubrovin M., Hewett J., Sena-Esteves M., Tan C.W., Slack M., Sadelain M., Breakefield X.O., Tjuvajev J.G. (1999). Functional coexpression of HSV-1 thymidine kinase and green fluorescent protein: implications for noninvasive imaging of transgene expression. Neoplasia.